# Copper(II) diacetyl-di(N^4^-methylthiosemicarbazone)

Chemical name: | Copper(II) diacetyl-di(N^4^-methylthiosemicarbazone)
Abbreviated name(s): | Cu-ATSM
Synonyms: | Diacetyl-bis(N^4^-methylthiosemicarbazone) copper(II)
Agent Category: | Compound
Target: | Hypoxic tissue
Target Category: | Redox trapping mechanism, reduction of Cu(II) to Cu(I)
Method of detection: | PET
Source(s) of signals: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[Pub (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20%28II%29%20diacetyl-di%28N%284%29-methylthiosemicarbazone%29%22%5BSubstance%20Name%5D)Med]

Hypoxia in malignant tumors can affect the outcome of anticancer treatments. Malignant tumors are relatively resistant to chemotherapy and irradiative therapy because of their lack of oxygen, which is a potent radiosensitizer. There is great interest in copper nuclides in nuclear medicine, which include isotopes with both diagnostic (^60,61,62,64^Cu) and therapeutic (^64,67^Cu) potential. Cu-ATSM has significant selectivity for hypoxic tissues in vivo and in vitro because of a reduction-oxidation (redox) trapping mechanism (1). Cu-ATSM accumulates avidly in hypoxic cells and delineates hypoxic areas within tumors, whereas it washes out in normoxic cells and in tissues where Cu-ATSM is not reduced and retained to the same extent (2-4).

The mechanism of retention of Cu-ATSM (with a redox potential of -297 mV) is a reduction of Cu(II) to Cu(I), followed by a loss of the radiometal from the complex. This reductive mechanism requires an intact enzymatic system of sequential electron transport chains (1, 5), which shows that the cells have an intact mitochondrial or microsomal electron transport system. Cu-ATSM accumulates mainly in the outer rims of tumor masses, which contain active tumor cells with high viability and high resistance to radiation therapy and to some chemotherapy treatments (6). For this reason, Cu-ATSM is regarded as a useful tool in positron emission tomography (PET) oncology.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20%28II%29%20diacetyl-di%28N%284%29-methylthiosemicarbazone%29%22%5BSubstance%20Name%5D%20AND%20%22synthesis%22%5BAll%20Fields%5D)]

One common method for synthesizing Cu-ATSM involves buffering CuCl_2_ in 1 M sodium acetate and then adding 15 µg of H_2_ATSM (1 mg/ml of Me_2_SO) and mixing for 2 min (1). The Cu-ATSM-containing solution is then washed with water, and Cu-ASTM is eluted in 0.1-ml fractions of ethanol. The radiochemical purity of the final Cu-ASTM solution is >98%.

Obata et al. (6) synthesized Cu-ATSM by mixing 4 ml of ^64^Cu-glycine solution with 0.2 ml of ATSM solution (0.5 mmol in Me_2_SO) with a radiochemical purity >99%, as determined by high-performance liquid chromatography (HPLC) on a reversed-phase column. Another method described by Petering et al. (7) uses 4-methyl-3-thiosemicarbazide and acetic acid as reagents. ^60,61,62,64^Cu can be produced using a generator system (for ^62^Cu) (8) or a biomedical cyclotron set up (for ^60,61,64^Cu) in regular PET centers (3, 9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20%28II%29%20diacetyl-di%28N%284%29-methylthiosemicarbazone%29%22%5BSubstance%20Name%5D%20AND%20%22in%20vitro%22%5BAll%20Fields%5D)]

Cu-ATSM uptake was shown to be dependent on the oxygen concentration (pO_2_) by in vitro studies, such as those performed by Dearling et al. (4, 10) on Chinese hamster ovary cells or by Lewis et al. (4) using the 9L gliosarcoma rat model. Cu-ATSM was evaluated in the EMT6 carcinoma cell line under various degrees of hypoxia and was compared with the flow tracer Cu-PTSM and the hypoxic tracer [^18^F]fluoromizonidazole. After 1 h, ^64^Cu-ATSM was taken up by EMT6 cells: 90% at 0 ppm, 77% at 1 x 10^3^ ppm, 38% at 5 x 10^3^ ppm, 35% at 5 x 10^4^ ppm, and 31% at 2 x 10^5^ ppm (11).

Other studies, such as the one by Obata et al. (5) that was performed on subcellular fractions obtained from Ehrlich ascites tumor cells, clarified the retention mechanism of Cu-ATSM in tumor cells and showed that Cu-ATSM was reduced mainly in the microsome/cytosol fraction rather than in the mitochondria—a completely different process from the one occurring in normal brain cells. The reduction process in the microsome/cytosol was found to be heat sensitive and was enhanced by adding exogenous NADPH, an indication of an enzymatic reduction of Cu-ATSM in tumor cells. Among the known bioreductive enzymes, NADH-cytochrome b5 reductase and NADPH-cytochrome P450 reductase in microsomes played major roles in the reductive retention of Cu-ATSM in tumors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20%28II%29%20diacetyl-di%28N%284%29-methylthiosemicarbazone%29%22%5BSubstance%20Name%5D%20AND%20%22rodentia%22%5BMeSH%5D)]

Cu-ATSM was shown to be dependent on the oxygen concentration, and uptake was heterogeneous in animal tumors (4). Several studies performed using rat heart models showed a selective trapping of Cu-ATSM in hypoxic tissues (3).

^60^Cu-ATSM was used to visualize hypoxia in a heart model of an occluded, acute left anterior descending (LAD) coronary artery by ex vivo tissue slicing, as described by Fujibayashi et al. (12). Studies conducted using the Langendorf isolated, perfused rat model showed that specific retention of Cu-ATSM was attributable to oxygen depletion. Cu-ATSM was shown to have a rapid washout from normally perfused, isolated rat hearts, whereas in ischemic hearts, there was a 3.5-fold retention of tracer within 15 min of tracer administration.

Systemic administration of ^64^Cu-ATSM showed a significant increase in survival time of hamsters bearing human GW39 colon cancer tumors. Radiotherapy experiments were performed in animals bearing either 7-day-old (0.5-1.0 g) or 15-day-old (1.5-2.0 g) tumors. The highest dose, 370 MBq (10 mCi) of ^64^Cu-ATSM, increased survival to 135 days in 50% of animals bearing 7-day-old tumors, 6-fold longer than the survival of control animals (20 days), with only transient leukopenia and thrombocytopenia but no overt toxicity (13).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20%28II%29%20diacetyl-di%28N%284%29-methylthiosemicarbazone%29%22%5BSubstance%20Name%5D%20AND%20%28%28%22dogs%22%5BMeSH%20Terms%5D%20OR%20dogs%5BText%20Word%5D%29)]

In studies performed on canine models of hypoxic myocardium, *Cu-ATSM PET (with *Cu defined as either ^60^Cu, ^61^Cu, or ^64^Cu) showed a quantitative selective uptake in hypoxic myocardium within 20 min of tracer administration (14).

Comparative studies of intratumoral distribution by ^64^Cu-ATSM and [^18^F]FDG on white Japanese rabbits (6) showed a major accumulation of ^64^Cu-ATSM around the outer rims of the tumor masses, which consisted mainly of active cells, whereas [^18^F]FDG was mainly accumulated in the inner regions, where pre-necrotic cells exist. Those results confirmed the superiority of ^64^Cu-ATSM for the detection of hypoxic but active tumor cell regions in vivo.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20%28II%29%20diacetyl-di%28N%284%29-methylthiosemicarbazone%29%22%5BSubstance%20Name%5D%20AND%20%28primates%20NOT%20human%29)]

No reference currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20%28II%29%20diacetyl-di%28N%284%29-methylthiosemicarbazone%29%22%5BSubstance%20Name%5D%20AND%20%22Humans%22%5BAll%20fields%5D)]

Human absorbed doses were calculated from hamster biodistributions; these data showed that the dose-critical organs were the lower large intestine (1.43 ± 0.19 rad/mCi) and the upper large intestine (1.20 ± 0.38 rad/mCi). Results varied from 0.072 rad/mCi for the urinary bladder to 1.430 rad/mCi for the lower large intestine. Experimental results from tumor-bearing hamsters suggested a dose of 277,500 MBq (7,500 mCi) of ^64^Cu-ATSM for clinical therapy trials in humans (13).

Takahashi et al. (15) performed PET with ^62^Cu-ATSM in 6 patients with lung cancer and demonstrated high tumor uptake of the tracer in all patients, although they did not correlate such uptake with response to therapy. Other studies of ^60^Cu-ATSM assessed by PET in patients with cervical cancer (16) and lung cancer (17) revealed clinically relevant information about tumor oxygenation that was predictive of tumor behavior and response to therapy. One of the studies was performed on 14 patients, all of whom had locally advanced cervical cancer with primary lesions >2.0 cm in diameter (1 with the International Federation of Gynecology and Obstetrics (FIGO) classification of clinical stage IB1, 1 with stage IB2, 8 with stage IIB, and 4 with stage IIIB), and the mean standardized uptake value for the primary tumors was 12.1 ± 5.5. The degree of tumor uptake of ^60^Cu-ATSM varied from 1.2 to 12.3 (Cu-ATSM/ tumor-to-muscle activity ratio); one patient was found with no discernable uptake (2).

In their study performed on patients with head and neck cancer, Chao et al. (18) showed that a novel Cu-ATSM-guided, intensity-modulated radiation therapy (IMRT) approach could escalate radiation dose in only selective hypoxic regions within the gross target volume without compromising the advantage of normal tissue sparing of IMRT. They developed a system to accurately co-register and merge hypoxia ^60^Cu-ATSM-PET and the therapeutic images for IMRT, with the aim of establishing a clinical-pathological correlation between ^60^Cu-ATSM retention and radiation therapy.

## References

1 Fujibayashi Y, Taniuchi H, Yonekura Y, Ohtani H, Konishi J, Yokoyama A. (1997). Copper-62-ATSM: a new hypoxia imaging agent with high membrane permeability and low redox potential. J Nucl Med.
2 Dearling JL, Lewis JS, Mullen GE, Welch MJ, Blower PJ. (2002). Copper bis(thiosemicarbazone) complexes as hypoxia imaging agents: structure-activity relationships. J Biol Inorg Chem.
3 McCarthy DW, Bass LA, Cutler PD, Shefer RE, Klinkowstein RE, Herrero P, Lewis JS, Cutler CS, Anderson CJ, Welch MJ. (1999). High purity production and potential applications of copper-60 and copper-61. Nucl Med Biol.
4 Lewis JS, Sharp TL, Laforest R, Fujibayashi Y, Welch MJ. (2001). Tumor uptake of copper-diacetyl-bis(N(4)-methylthiosemicarbazone): effect of changes in tissue oxygenation. J Nucl Med.
5 Obata A, Yoshimi E, Waki A, Lewis JS, Oyama N, Welch MJ, Saji H, Yonekura Y, Fujibayashi Y. (2001). Retention mechanism of hypoxia selective nuclear imaging/radiotherapeutic agent cu-diacetyl-bis(N4-methylthiosemicarbazone) (Cu-ATSM) in tumor cells. Ann Nucl Med.
6 Obata A, Yoshimoto M, Kasamatsu S, Naiki H, Takamatsu S, Kashikura K, Furukawa T, Lewis JS, Welch MJ, Saji H, Yonekura Y, Fujibayashi Y. (2003). Intra-tumoral distribution of (64)Cu-ATSM: a comparison study with FDG. Nucl Med Biol.
7 Petering HG, Buskirk HH, Underwood GE. (1964). The Anti-Tumor Activity Of 2-Keto-3-Ethoxybutyraldehyde Bis(Thiosemicarbazone) And Related Compounds. Cancer Res.
8 Fujibayashi Y, Matsumoto K, Yonekura Y, Konishi J, Yokoyama A. (1989). A new zinc-62/copper-62 generator as a copper-62 source for PET radiopharmaceuticals. J Nucl Med.
9 Obata A, Kasamatsu S, McCarthy DW, Welch MJ, Saji H, Yonekura Y, Fujibayashi Y. (2003). Production of therapeutic quantities of (64)Cu using a 12 MeV cyclotron. Nucl Med Biol.
10 Dearling JL, Lewis JS, Mullen GE, Rae MT, Zweit J, Blower PJ. (1998). Design of hypoxia-targeting radiopharmaceuticals: selective uptake of copper-64 complexes in hypoxic cells in vitro. Eur J Nucl Med.
11 Lewis JS, McCarthy DW, McCarthy TJ, Fujibayashi Y, Welch MJ. (1999). Evaluation of 64Cu-ATSM in vitro and in vivo in a hypoxic tumor model. J Nucl Med.
12 Fujibayashi Y, Cutler CS, Anderson CJ, McCarthy DW, Jones LA, Sharp T, Yonekura Y, Welch MJ. (1999). Comparative studies of Cu-64-ATSM and C-11-acetate in an acute myocardial infarction model: ex vivo imaging of hypoxia in rats. Nucl Med Biol.
13 Lewis J, Laforest R, Buettner T, Song S, Fujibayashi Y, Connett J, Welch M. (2001). Copper-64-diacetyl-bis(N4-methylthiosemicarbazone): An agent for radiotherapy. Proc Natl Acad Sci U S A.
14 Lewis JS, Herrero P, Sharp TL, Engelbach JA, Fujibayashi Y, Laforest R, Kovacs A, Gropler RJ, Welch MJ. (2002). Delineation of hypoxia in canine myocardium using PET and copper(II)-diacetyl-bis(N(4)-methylthiosemicarbazone). J Nucl Med.
15 Takahashi N, Fujibayashi Y, Yonekura Y, Welch MJ, Waki A, Tsuchida T, Sadato N, Sugimoto K, Itoh H. (2000). Evaluation of 62Cu labeled diacetyl-bis(N4-methylthiosemicarbazone) as a hypoxic tissue tracer in patients with lung cancer. Ann Nucl Med.
16 Dehdashti F, Grigsby PW, Mintun MA, Lewis JS, Siegel BA, Welch MJ. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
17 Dehdashti F, Mintun MA, Lewis JS, Bradley J, Govindan R, Laforest R, Welch MJ, Siegel BA. (2003). In vivo assessment of tumor hypoxia in lung cancer with 60Cu-ATSM. Eur J Nucl Med Mol Imaging.
18 Chao KS, Bosch WR, Mutic S, Lewis JS, Dehdashti F, Mintun MA, Dempsey JF, Perez CA, Purdy JA, Welch MJ. (2001). A novel approach to overcome hypoxic tumor resistance: Cu-ATSM-guided intensity-modulated radiation therapy. Int J Radiat Oncol Biol Phys.